# Doxorubicin-loaded poly(ethylene oxide)-trimellitic anhydride chloride-folate superparamagnetic iron oxide nanoparticles

Chemical name: | Doxorubicin-loaded poly(ethylene oxide)-trimellitic anhydride chloride-folate superparamagnetic iron oxide nanoparticles
Abbreviated name: | YCC-DOX
Synonym:
Agent Category: | Nanoparticles
Target: | Folate receptor (FR)
Target Category: | Receptor
Method of detection: | Magnetic resonance imaging
Source of signal / contrast: | Superparamagnetic iron oxide
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=doxorubicin%20loaded%20superparamagnetic%20iron%20oxide%20nanoparticles&cmd=DetailsSearch)]

Because of low specificity, many cancer therapeutic agents (most small molecules and some targeted biopharmaceuticals) used to treat malignancies often have severe systemic toxicity and other undesirable side effects in a patient (1, 2). Therefore, to reduce the toxicity and side effects of an anticancer drug, either the chemical structure of the compound has to be altered or a drug delivery system must be used to specifically target the drug to affected organs or tissues such that the surrounding normal tissues are not affected by the antineoplastic agent. Investigators have developed and evaluated various nanocarrier drug delivery systems, including nanoparticles (NPs), to target and deliver drugs for the detection, treatment, and imaging of diseased tissues and organs up to the cellular level (3). Doxorubicin (DOX) is an anthracycline-based antibiotic that is used as an antineoplastic agent against several different cancers types, but its application in the clinic is limited by the dose-dependent cardiotoxicity and cytotoxicity observed in many patients (4). As a consequence, a pegylated liposomal NP preparation of DOX (PLD) was developed and shown to have a long blood circulation half-life (2–3 days versus 5 min for free DOX) and had a very high accumulation in tumors compared to the normal surrounding tissue. In addition, PLD alone had a superior treatment outcome (in comparison to DOX used at the same concentration in combination with two other chemotherapeutic agents) and showed lower toxicity (5). Anticancer drugs have also been encapsulated in different types of NPs, such as superparamagnetic iron oxide (SPIO) NPs, that are conjugated to target-seeking molecules, bind only to cells that produce the appropriate biomarker, are used as magnetic resonance imaging (MRI) contrast agents, and serve as multifunctional drug delivery and imaging agents (6). The structure, biological characteristics, and therapeutic and imaging applications of SPIOs are described elsewhere (7).

Maeng et al. synthesized a polymeric NP that contained DOX and an SPIO and evaluated the efficacy of the NPs, designated YCC-DOX, as a targeted therapeutic agent against hepatic cancer and as an MRI agent in rats and rabbits having liver cancer lesions induced by diethylnitrosamine (DEN; has carcinogenic and mutagenic properties) and O-ethyl O-2-diisopropylaminoethyl methylphosphonite (VX2; a nerve agent), respectively (8). The NP contained poly(ethylene oxide)-trimellitic anhydride chloride-folate, where the folate component serves as the tumor-targeting molecule because it has a very high affinity (K_d_, ~10^-10^ M) for the folate receptor (FR). Also, the FR is overexpressed in many human cancers, and the FR-folate structure is rapidly internalized by the cell through endocytosis, resulting in targeted delivery of the drug to the tumor cells (8).

### Other Sources of Information Related to Folate Receptor

Adult human FR protein and mRNA sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_016724.2).

Human FR gene. (http://www.ncbi.nlm.nih.gov/gene/2348) (Gene ID: 2348)

FR Clinical trials (http://clinicaltrials.gov/ct2/results?term=folate+receptor+AND+targeted+AND+cancer).

FR in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/136430) database.

FR pathway in Kyoto Encyclopedia of Genes and Genomes (KEGG). (http://www.genome.jp/dbget-bin/show_pathway?hsa04144+2348)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=YCC-DOX%20synthesis&cmd=DetailsSearch)]

The synthesis of folate containing YCC-DOX has been described by Maeng et al. (8). The net yield of the NP after synthesis was reported to be 85–94 mol percent based on the amount of folic acid incorporated (8). The NPs were determined to contain 2.1 mg/mL DOX and 2.5 mg/mL iron. The average diameter of the YCC-DOX NP was 84.7 nm as determined with a submicron particle size analyzer and transmission electron microscopy revealed that the particles had a spherical shape.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=YCC-DOX%20in%20vitro&cmd=DetailsSearch)]

The release of DOX from YCC-DOX was investigated under in vitro conditions as described by Maeng et al. (8). At pH 5.1 and 7.4, approximately 56% and 33% DOX, respectively, was released from the NPs within 24 h, indicating that the NPs were relatively stable at a physiological pH. This study indicated that the rate of DOX release from the NPs was almost two-fold higher at the acidic pH (e.g., as found in the endosomes and the lysosomes of tumor cells) than at physiological pH.

For competitive inhibition studies, the cellular uptake of YCC-DOX was studied by separately exposing Hep3B (a human hepatocellular carcinoma (http://www.cdph.ca.gov/programs/ccr/Documents/HepatocellularCarcin-10-14-09.pdf) cell line that overexpresses the FR) and KB cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-17&Template=cellBiology) to YCC-DOX NPs with or without FA pretreatment (2 mM) for competitive inhibition (8). The uptake of YCC-DOX NPs was visualized with a confocal laser scanning microscope, and both cell types pretreated with DOX were shown to have a reduced uptake of the NPs compared to the untreated cells.

The cytotoxicity of YYC-DOX NPs was compared to that of free DOX (FD) and a commercially available liposomal preparation of DOX (http://www.kodc.or.kr/cmed/down/DOXIL_PI.pdf) (CD) using Hep3B cells (8). The cells were exposed to the different preparations of DOX, and cell viability was determined using the 3-(4,5-dimethylthiazol-2-yl)-2,5-diphenyltetrazolium bromide assay (also known as the MTT assay) at 24 h and 48 h after exposure to DOX. At both time points, YCC-DOX NPs were shown to reduce the cell viability from 100% to ~50% and ~20% at 24 h and 48 h, respectively, at a concentration of 100 μM DOX, similar to results with FD. However, with CD the cell viability remained >80% at these time points at the same concentration of DOX.

In another in vitro study, the MRI signals of YCC and YCC-DOX (at iron concentrations of 0–25 μg/mL) from T2-weighted images acquired at a 1.5-T, fast spin echo, with a TR ¼ 3,600 ms and TE ¼ 88.6 ms, were shown to be higher than a commercially available liver-specific MRI contrast agent (http://radiologie-uni-frankfurt.de/sites/radiologie-uni-frankfurt.de/content/e43/e2321/e2331/resofinal_eng.pdf) at the same iron concentrations (8).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=YCC-DOX%20rodentia&cmd=DetailsSearch)]

DEN-Treated rats with hepatic cancer were divided into four drug treatment groups as follows: saline-treated (n = 6 animals; this was the control group), FD-treated (n = 10 animals), CD-treated (n = 10 animals), and YCC-DOX–treated (n = 10 animals) (8). The animals in each group were intravenously injected through the tail vein with the respective drug preparations (2 mg DOX equivalent/kg body weight) three times at 5-day intervals (days 0, 5, and 10). The tumor volumes, the relative volumes, signal intensity (using MRI), and normalized signal intensity of animals in the different groups were measured or calculated on day 0 and day 20 as described by Maeng et al. (8). In the YCC-DOX–treated animals, the relative volumes of the tumors were reported to decrease by 19.3-, 3.5-, and 4.5-fold compared to the rats treated with saline, FD (P < 0.05), and CD (P < 0.002), respectively. No blocking studies were reported.

In another experiment, MRI was performed on rats with DEN-induced hepatic tumors (number of animals not specified) and intravenously injected with the same volume of either YCC, YCC-DOX (each containing 2.5 mg iron/mL), or contrast agent (containing 27.9 mg iron/mL). T2- or T2*-Weighted images were acquired using either a 1.5-T, fast spin echo, with a TR and TE of ¼ 3,600 ms and ¼ 83.5 ms, respectively, or a 1.5-T, gradient-recalled echo, with a TR and TE of ¼ 30 ms and ¼ 13.9 ms, respectively. The animals were imaged before and after an intravenous injection of the agents and a decrease in the tumor signal intensity of the YCC-DOX–treated rats was noted to be significantly higher (P value not provided) than the contrast agent–treated animals as determined from the T2-weighted images. In addition, the signal intensities obtained from the YCC- and the YCC-DOX–treated animals were reduced by ~40% compared to the other treatments. No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=YCC-DOX%20other%20non-primate%20mammals&cmd=DetailsSearch)]

In a study similar to that performed with the rats (see above), rabbits (n = 6–10 animals/group) bearing VX2-induced hepatic tumors were treated with the various preparations of DOX as listed above, including a saline-treated control group (8). Subsequently, relative volume values were obtained from the rabbits as detailed above, and it was shown that the values decreased 21.5-, 2.4- and 3.5-fold in the YYC-DOX–treated animals compared to animals in the saline-, FD-, and CD-treated groups, respectively. This indicated that the effect of the YCC-DOX preparation in rabbits bearing the VX2-induced tumors was similar to that observed with rats bearing the DEN-induced hepatic tumors. No blocking studies were reported.

The YCC-DOX–treated rabbits showed little cardiac toxicity, oral mucositis, or hair loss compared to the animals treated with FD and CD (8). The mortality rate of animals treated with the FD and CD preparation was nearly 10% and 33%, respectively, compared with 0% for the YCC-DOX–treated rabbits.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=YCC-DOX%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=YCC-DOX%20Human%20studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Albini A., Pennesi G., Donatelli F., Cammarota R., De Flora S., Noonan D.M. (2010). Cardiotoxicity of anticancer drugs: the need for cardio-oncology and cardio-oncological prevention. J Natl Cancer Inst.
2 Randall L.M., Monk B.J. (2010). Bevacizumab toxicities and their management in ovarian cancer. Gynecol Oncol.
3 Bhaskar S., Tian F., Stoeger T., Kreyling W., de la Fuente J.M., Grazu V., Borm P., Estrada G., Ntziachristos V., Razansky D. (2010). Multifunctional Nanocarriers for diagnostics, drug delivery and targeted treatment across blood-brain barrier: perspectives on tracking and neuroimaging. Part Fibre Toxicol.
4 Carvalho C., Santos R.X., Cardoso S., Correia S., Oliveira P.J., Santos M.S., Moreira P.I. (2009). Doxorubicin: the good, the bad and the ugly effect. Curr Med Chem.
5 Gaitanis A., Staal S. (2010). Liposomal doxorubicin and nab-paclitaxel: nanoparticle cancer chemotherapy in current clinical use. Methods Mol Biol.
6 Islam T., Josephson L. (2009). Current state and future applications of active targeting in malignancies using superparamagnetic iron oxide nanoparticles. Cancer Biomark.
7 Tanimoto A., Kuribayashi S. (2006). Application of superparamagnetic iron oxide to imaging of hepatocellular carcinoma. Eur J Radiol.
8 Maeng J.H., Lee D.H., Jung K.H., Bae Y.H., Park I.S., Jeong S., Jeon Y.S., Shim C.K., Kim W., Kim J., Lee J., Lee Y.M., Kim J.H., Kim W.H., Hong S.S. (2010). Multifunctional doxorubicin loaded superparamagnetic iron oxide nanoparticles for chemotherapy and magnetic resonance imaging in liver cancer. Biomaterials.